# [^111^In-Diethylenetriamine pentaacetic acid-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]bombesin(5-14)

Chemical name: | [^111^In-Diethylenetriamine pentaacetic acid-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]bombesin(5-14)
Abbreviated name: | [^111^In-DTPA- ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]BN(5-14)
Synonym: | ^111^In-BN analog, ^111^In-BBN analog
Agent Category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRP-R)
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | [^111^In-DTPA- ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]BN(5-14). The ^111^In coordination configuration has not been established by experiments. Click on PubChem (http://pubchem.ncbi.nlm.nih.gov) (SID:46501389 (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?sid=46501389)) for additional information. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=55584176), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=2925&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about BN and GRP.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Radiolabeled+Bombesin+analog+OR+(DTPA)-BN)]

[^111^In-Diethylenetriamine pentaacetic acid-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-bombesin(5-14) ([^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14)) is a peptide analog of the human gastrin-releasing peptide (GRP) conjugated with ^111^In, and it was developed for single-photon emission computed tomography (SPECT) imaging of tumors with overexpressed GRP receptors (GRP-R) (1). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The amphibian bombesin (BN or BBN), a peptide of 14 amino acids, is an analog of human GRP, a peptide of 27 amino acids, which binds to GRP-R with high affinity and specificity (2, 3). Both GRP and BN share an amidated C-terminus sequence homology of seven amino acids, -Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system (4, 5). They also act as potential growth factors for both normal and neoplastic tissues. Specific BN receptors (BN-R) have been identified in CNS and GI tissues and in a number of tumor cell lines. The BN-R superfamily includes at least four different subtypes, namely the GRP-R subtype (BB2), the neuromedin B receptor subtype (BB1), the BB3 subtype, and the BB4 subtype (8). Overexpression of GRP-R in various human tumors (e.g., breast, prostate, lung, colon, ovarian, and pancreatic cancers) provides opportunities to image tumors with the use of specific molecular imaging agents designed to target the GRP-R (3, 6-9).

There have been varying degrees of success in the development of GRP-R–targeted radiopharmaceuticals for diagnostic or therapeutic applications (9). Various BN analogs have been labeled with ^99m^Tc and ^111^In for SPECT imaging (13, 14). Despite some concern about the possible tumor growth–stimulatory effect of BN, Breeman et al. (10) synthesized the BN-R agonist [^111^In-DTPA-Pro^1^,Tyr^4^]BN. The study reported that this agonist had a high specific localization in GRP-R–positive tissues and tumors. [^111^In-DTPA-Pro^1^,Tyr^4^]BN differs from native BN in that pGlu^1^ is replaced with DTPA-Pro^1^ and Leu^4^ is replaced with Tyr^4^. Breeman et al. (10) showed that this agonist was internalized by GRP-R–expressing cells, whereas the antagonist ([^111^In-DTPA-Tyr^5^,D-Phe^6^]BN(5-13)NHEt) was not. On the basis of this finding, de Visser et al. (1) developed new DTPA-couple BN analogs with shortened amino acid sequences containing non-natural amino acid derivatives to improve the receptor binding affinity of the compounds. [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) is one of the tested radioactive probes that appears to be a promising candidate for use in molecular imaging of tumors expressing GRP-R (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeled+Bombesin+analog+OR+(DTPA)-BN)+AND+synthesis)]

The BN peptide analog 4-aminocarboxymethylpiperidine [ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14), was synthesized using the solid-phase method according to the Fmoc strategy and Rink amide resin (1). A solid-phase peptide synthesizer was used. The protocol required 25 μmol of starting resin and 75 μmol of subsequent Fmoc-protected amino acids activated by the combination of N-hydroxybenzotriazole and (2-(1-H-benzotriazol-1-yl)-1,1,3,3-tetramethyluronium hexafluorophosphate. Coupling of DTPA to [ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) was performed by placing tributyl-DTPA at the appropriate location in an amino acid column. Cleavage and deprotection were accomplished using a mixture of 85% trifluoroacetic acid, 5% thioanisole, 5% phenol, and 5% water. The crude peptide was precipitated with t-butyl methyl ether and purified by reverse-phase, high-performance liquid chromatography (HPLC). The molecular weight of the peptide was determined by mass spectrometry to be 1,644.7 (M+H) as compared to the theoretical value of 1,644. Radiolabeling of [ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) with ^111^In used the same procedure as described by Bakker et al. (11). A 40- to 70-molar excess of peptide over ^111^In was used. The peptide in 0.01–0.1 M acetic acid was mixed with ^111^In in 0.04–0.05 M hydrochloric acid. The reaction mixture was incubated at room temperature for 10 min. The labeling yield and radiochemical purity were >95% as determined by instant thin-layer chromatography and reverse-phase chromatography on C18 Sep-Pak column. The maximum specific activity was 200 MBq/nmol (5.4 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(in+vitro))]

De Visser et al. (1) determined the receptor affinity of [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) using frozen sections of the GRP-R–expressing human prostate tumor xenograft PC-295 and rat colon. In vitro autoradiography was conducted by incubating 10-μm sections for 1 h at room temperature with 0.1 nM of the radiolabeled BN analog. The sections were incubated with increasing amounts of the nonradioactive BN analog to generate the competitive inhibition curve. The 50% inhibitory concentration (IC_50_) was determined to be 0.08 ± 0.01 nM on the rat colon tissue and 0.36 ± 0.01 nM on the human PC-295 tissue. De Visser et al. (1) also reported an IC_50_ value of 1.3 nM for a primary human prostate cancer section. In comparison, the IC_50_ values for [^111^In-DTPA-Pro^1^,Tyr^4^]BN were 2.28 ± 0.57 nM and 1.40 ± 0.07 nM for the rat colon and human PC-295, respectively.

De Visser et al. (1) studied the cell internalization of [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) in the rat pancreatic tumor cell line CA20948 and human prostate tumor cell line PC3. The radioligand had the highest rate of internalization in the first hour of incubation. Extrapolated from Figure 2a of de Visser et al. (1), the internalization, expressed as a percentage of the injected dose per mg cellular protein (% ID/mg) of the radioligand, in the CA20948 cells was ~26% ID/mg at 60 min and ~32% ID/mg at 180 min. In comparison, the internalization of [^111^In-DTPA-Pro^1^,Tyr^4^]BN was ~11% ID/mg and ~23% ID/mg at 60 min and 180 min, respectively. The cell internalization was different in the PC3 cells. Extrapolated from Figure 2b of de Visser et al. (1), [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) was internalized ~6% ID/mg at 60 min and ~7.75% ID/mg at 180 min. In comparison, the internalization of [^111^In-DTPA-Pro^1^,Tyr^4^]BN was ~5% ID/mg and ~7% ID/mg at 60 min and 180 min, respectively. When a blocking study was performed by adding increased amounts of unlabeled [Tyr^4^]BN to the incubating medium that contained 10^–10^ M of the radioactive probe, the results showed that the addition of 1–10 nM of unlabeled [Tyr^4^]BN effectively blocked the internalization of [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14).

An in vitro serum stability study of [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) using HPLC analysis showed that the percentage of intact radiolabeled peptide was 74% after incubation in human serum for 4 h at 37ºC (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(rodentia))]

Biodistribution studies of [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) were performed in Lewis rats bearing a rat pancreatic tumor CA20948 (area = 2–4 cm^2^) and nude mice bearing a human prostate tumor PC3 (area = 1 cm^2^) (1). The dose of [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) for each rat or mouse was 2–4 MBq/0.1 μg (54–108 μCi/0.1 μg) of radiolabeled peptide or 2–4 MBq/0.06 pmol (54–108 μCi/0.06 pmol) of radiolabeled peptide on the basis of the peptide’s molecular weight of 1,644. In the rats with a CA20948 tumor, the tumor radioactivity levels (n = 3–27) in percentage injected dose per gram (% ID/g) were 0.583 ± 0.244 (4 h), 0.521 ± 0.115 (24 h), 0.277 ± 0.167 (48 h), and 0.266 ± 0.082 (72 h). The pancreas and bowel (stomach, small intestine, caecum, and colon) also had relatively high radioactivity levels. The tumor/blood ratios were 49, 74, 92, and 133 for 4 h, 24 h, 48 h, and 72 h, respectively. The tumor/muscle ratios were 146, 130, 69, and 89 for 4 h, 24 h, 48 h, and 72 h, respectively. The tumor/kidney ratios were 0.5, 0.4, 0.3, and 0.4 for 4 h, 24 h, 48 h, and 72 h, respectively. In comparison, the tumor/normal tissue radioactivity ratios (n = 6) at 4 h for ^111^In-DTPA-Pro^1^,Tyr^4^]BN were 50 (tumor/blood), 126 (tumor/muscle), and 0.2 (tumor/kidney). When a blocking dose of 100 μg [Tyr^4^]BN (n = 20) was co-injected, the tumor radioactivity level decreased from 0.583 ± 0.244% ID/g to 0.067 ± 0.088% ID/g at 4 h, and the pancreas radioactivity level was reduced from 2.883 ± 1.135% ID/g to 0.185 ± 0.520% ID/g. The bowel radioactivity levels were all decreased. For the mice with a PC3 tumor (n = 11), the tumor radioactivity level was 0.839 ± 0.577% ID/g at 4 h and was reduced to 0.120 ± 0.122% ID/g (n = 7) with a co-injection dose of 50 μg [Tyr^4^]BN. The tumor/normal tissue radioactivity ratios at 4 h were 18 (tumor/blood), 49 (tumor/muscle), and 0.8 (tumor/kidney). The pancreas radioactivity level was 15.010 ± 3.930% ID/g at 4 h and was reduced to 0.553 ± 0.312% ID/g by [Tyr^4^]BN. The bowel radioactivity levels were also reduced by the blocking dose. In comparison, the [^111^In-DTPA-Pro^1^,Tyr^4^]BN had 4-h tumor/normal tissue ratios of 28 (tumor/blood), 36 (tumor/muscle), and 0.1 (tumor/kidney).

A tumor-imaging study was conducted in one rat bearing a CA20948 tumor (right flank) and a GRP-R–positive rat pancreatic tumor AR42J (left flank) (1). A rat received a [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) dose of 4 MBq/0.1 μg (108 μCi/0.1 μg) radiolabeled peptide or 4 MBq/0.06 pmol radiolabeled peptide on the basis of the peptide’s molecular weight of 1,644. In this study, the radioactivity level in the AR42J tumor was readily detectable at 1 min, and the background radioactivity rapidly decreased after 1 h. At 4 h, the tumor/normal tissue radioactivity ratios were 85 (tumor/blood), 145 (tumor/muscle), and 0.58 (tumor/kidney). However, the radioactivity in the CA20948 tumor was relatively lower with tumor/normal tissue ratios of 34 (tumor/blood), 58 (tumor/muscle), and 0.23 (tumor/kidney) at 4 h. De Visser et al. (1) suggested that the lower radioactivity tumor level was a result of necrosis in the large CA20948 tumor and a higher GRP-R density for the AR42J tumor. When a microSPECT/CT study was performed in one nude mouse bearing a CA20948 tumor on the shoulder with a [^111^In-DTPA-ACMpip^5^,Tha^6^,βAla^11^,Tha^13^,NIe^14^]-BN(5-14) dose of 10 MBq/0.1 μg (0.27 mCi/μg) or 10 MBq/0.06 pmol (0.27 mCi/0.06 pmol), the tumor radioactivity level was much higher than that in the rat bearing the tumor. At 4 h, the tumor/blood ratio was 99, the tumor/muscle ratio was 234, and the tumor/kidney ratio was 3.5. The sagittal, coronal, and transaxial slices showed a clear localization of the tumor with no interfering background.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DTPA)-BN))+AND+(humans))]

No publication is currently available.

## References

1. de Visser, M., H.F. Bernard, J.L. Erion, M.A. Schmidt, A. Srinivasan, B. Waser, J.C. Reubi, E.P. Krenning, and M. de Jong, Novel (111)In-labelled bombesin analogues for molecular imaging of prostate tumours. Eur J Nucl Med Mol Imaging, 2007.
2 Smith C.J., Gali H., Sieckman G.L., Higginbotham C., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of (99m)Tc-N(3)S-X-BBN[7-14]NH(2): an in vitro/in vivo structure-activity relationship study where X = 0-, 3-, 5-, 8-, and 11-carbon tethering moieties. Bioconjug Chem.
3 Ma L., Yu P., Veerendra B., Rold T.L., Retzloff L., Prasanphanich A., Sieckman G., Hoffman T.J., Volkert W.A., Smith C.J. (2007). In Vitro and In Vivo Evaluation of Alexa Fluor 680-Bombesin[7-14]NH(2) Peptide Conjugate, a High-Affinity Fluorescent Probe with High Selectivity for the Gastrin-Releasing Peptide Receptor. Mol Imaging.
4 Mantey S., Frucht H., Coy D.H., Jensen R.T. (1993). Characterization of bombesin receptors using a novel, potent, radiolabeled antagonist that distinguishes bombesin receptor subtypes. Mol Pharmacol.
5 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Biddlecombe G.B., Rogers B.E., de Visser M., Parry J.J., de Jong M., Erion J.L., Lewis J.S. (2007). Molecular imaging of gastrin-releasing peptide receptor-positive tumors in mice using 64Cu- and 86Y-DOTA-(Pro1,Tyr4)-bombesin(1-14). Bioconjug Chem.
8 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
9 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
10 Breeman W.A., Hofland L.J., de Jong M., Bernard B.F., Srinivasan A., Kwekkeboom D.J., Visser T.J., Krenning E.P. (1999). Evaluation of radiolabelled bombesin analogues for receptor-targeted scintigraphy and radiotherapy. Int J Cancer.
11 Bakker W.H., Albert R., Bruns C., Breeman W.A., Hofland L.J., Marbach P., Pless J., Pralet D., Stolz B., Koper J.W., et al. (1991). [111In-DTPA-D-Phe1]-octreotide, a potential radiopharmaceutical for imaging of somatostatin receptor-positive tumors: synthesis, radiolabeling and in vitro validation. Life Sci.